# ^124^I-Labeled antibody against lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)

Chemical name: | ^124^I-Labeled antibody against lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)
Abbreviated name: | ^124^I-Anti-LYVE-1
Synonym:
Agent category: | Antibody
Target: | Lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LYVE-1)]

The primary function of the lymphatic system is to drain ~10% of the interstitial fluid from small capillaries to lymphatic vessels through lymph nodes (LNs) and finally to the venous system (1-5). LNs form a natural filter for lymphatic drainage and prevent the possible migration of cancer cells from the lymphatic system into the body. As the first LN that receives lymph drainage from a tumor bed, the sentinel LN is very likely to contain cancer cells if the primary tumor has spread via the lymphatic system (1, 2). The lymphatic system is complex, and its detection and mapping remain challenging (1, 2, 6, 7). However, with advances of new imaging agents and techniques, imaging and mapping of both the lymphatic vessels and the LNs are now possible with x-ray–computed tomography, ultrasound, nuclear medicine, and magnetic resonance imaging (7-9). There is increasing evidence that tumor cells induce lymphangiogenesis in tumor-draining LNs in experimental models of cancer (10, 11) as well as in LNs of patients with metastatic melanoma and breast cancer (12, 13). Therefore, LN lymphangiogenesis might provide a target to image the early stages of tumor metastasis. In addition, chronic inflamed tissues produce vascular endothelial growth factor (VEGF) to induce lymphangiogenesis in draining LNs.

Hyaluronan (HA) is an abundant extracellular matrix glycosaminoglycan in skin and mesenchymal tissues, where it facilitates cell migration during inflammation, wound healing, metastasis, and embryonic morphogenesis (14, 15). CD44 is an integral cell membrane glycoprotein on leukocytes and has an important role in matrix adhesion lymphocyte activation and LN homing (16). CD44 binds HA to induce extravasation of lymphoid cells. Lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1) has a 41% homology to CD44, and LYVE-1 expression is largely restricted to endothelial cells of lymphatic vessels and splenic sinusoidal endothelial cells. Expression was undetectable on lymphocytes, hematopoietic cells, or vascular endothelial cells. Mumprecht et al. (17) used ^124^I-labeled antibody against LYVE-1 (^124^I-anti-LYVE-1) for in vivo imaging of inflammation- and tumor-induced LN lymphangiogenesis with positron emission tomography (PET).

### Related Resource Links:

- Chapters in MICAD (LYVE-1 (http://www.ncbi.nlm.nih.gov/books?term=LYVE-1%20AND%20micad%5Bbook%5D), CD44 (http://www.ncbi.nlm.nih.gov/books?term=CD44%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (LYVE-1 (http://www.ncbi.nlm.nih.gov/gene/10894), CD44 (http://www.ncbi.nlm.nih.gov/gene/960))
- Articles in Online Mendelian Inheritance in Man (OMIM) (LYVE-1 (http://www.ncbi.nlm.nih.gov/omim/605702), CD44 (http://www.ncbi.nlm.nih.gov/omim/107269))
- Clinical trials (LYVE-1 (http://www.clinicaltrials.gov/ct2/show/NCT00748657?term=LYVE1&rank=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iodine%20LYVE-1%20AND+synthesis)]

Anti-mouse LYVE-1 rat antibody (~1.2 nmol, clone 223322, R&D Systems) was labeled with 2.7 MBq (0.073 mCi) Na^124^I in the presence of chloramine T for 2 min at room temperature (17). ^124^I-Anti-LYVE-1 was isolated with size-exclusion column chromatography, with a radiochemical purity of >95% and a specific activity of 3.7 MBq/nmol (0.1 mCi/nmol). ^125^I-Anti-LYVE-1 antibody was prepared similarly with a radiochemical purity of >99% and a specific activity of 12.8 MBq/nmol (0.35 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iodine%20LYVE-1%20AND+in+vitro)]

^124^I-Anti-LYVE-1 and ^125^I-anti-LYVE-1 exhibited immunoreactivity of 92%–94% (17). Unlabeled anti-LYVE-1 inhibited binding of ^124^I-anti-LYVE-1 and ^125^I-anti-LYVE-1 to immobilized mouse LYVE-1 with IC_50_ values of 26 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iodine%20LYVE-1+AND+rodentia)]

Mumprecht et al. (17) applied oxazolone to one ear to induce LN lymphangiogenesis in female hemizygous transgenic K14/VEGF mice that overexpress VEGF-A in the epidermis. K14/VEGF mice developed a chronic ear skin inflammation that resulted in lymphangiogenesis in the ear skin and in the ear-draining (auricular) LNs 6–8 days after oxazolone application. Intravenous injection of 0.05 nmol (n = 5 mice), 0.25 nmol (n = 5 mice), or 0.60 nmol (n = 3 mice) ^125^I-anti-LYVE-1 in these mice showed a dose-dependent accumulation of radioactivity in the excised inflamed auricular LNs but not in the control auricular LNs in 1 d after injection. Accumulation in the inflamed auricular LNs increased 1.9-, 4.6-, and 4.6-fold over accumulation in the control auricular LNs for 0.05, 0.25, and 0.60 nmol ^125^I-anti-LYVE-1, respectively. Accumulation of control ^125^I-IgG was less than that of ^125^I-anti-LYVE-1 in both auricular LNs. Pretreatment with excess unlabeled anti-LYVE-1 (4.5 nmol, 1 d) reduced accumulation of ^125^I-anti-LYVE-1 by ~70% in both auricular LNs at 1 d after injection. Microradiography of tissue sections showed localization of ^125^I-anti-LYVE-1 at vessel-like structures in the draining LNs, ears, lungs, and intestines. Analysis of serum at 4, 24, and 52 h after ^125^I-anti-LYVE-1 injection showed that most of the ^125^I-anti-LYVE-1 was intact with a small amount of free ^125^I. PET imaging with 0.2 nmol ^124^I-anti-LYVE-1 showed radioactivity localization in the auricular, brachial, and axillary LNs in mice (n = 2) with LN lymphangiogenesis at 1 d after injection. The inflamed auricular LNs produced stronger signals than the contralateral auricular LNs. Control ^124^I-IgG remained mainly in the blood with little signal from LNs.

In another study, PET imaging was performed in a tumor-induced LN lymphangiogenesis in mice bearing B16-F1-VEGF-C tumors in the left footpad (17). In mice injected with ^124^I-anti-LYVE-1 (n = 2), tumor-draining popliteal LNs were clearly visualized at 24 h after injection. There were 4.1- to 5.5-fold increases in ^124^I-anti-LYVE-1 accumulation in the tumor-draining LNs compared with control LNs. In mice (n = 4) bearing B16-F10-luc2-VEGF-C tumors, bioluminescence imaging showed three mice with strong signal and one mouse with weak signal in the tumor-draining LNs, indicating the presence of metastases in all four mice. [^18^F]-FDG PET imaging on the following day showed radioactivity in the region of the tumor-draining LNs in only one mouse. On the other hand, ^124^I-anti-LYVE-1 PET imaging performed 1 day later detected radioactivity in the region of the tumor-draining LNs in all four mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iodine%20LYVE-1+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iodine%20LYVE-1+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iodine%20LYVE-1%20AND+human)]

No publication is currently available.

## NIH Support

R01 CA69184

## References

1 Clement O., Luciani A. (2004). Imaging the lymphatic system: possibilities and clinical applications. Eur Radiol.
2 Styblo T., Aarsvold J.N., Grant S.F., Cohen C., Larsen T., Waldrop S., Alazraki N.P. (2001). Sentinel lymph nodes: optimizing success. Semin Roentgenol.
3 Hoh C.K., Wallace A.M., Vera D.R. (2003). Preclinical studies of [(99m)Tc]DTPA-mannosyl-dextran. Nucl Med Biol.
4 Salem C.E., Hoh C.K., Wallace A.M., Vera D.R. (2006). A preclinical study of prostate sentinel lymph node mapping with [99mTC]diethylenetetramine pentaacetic acid-mannosyl-dextran. J Urol.
5 Vera D.R., Wallace A.M., Hoh C.K., Mattrey R.F. (2001). A synthetic macromolecule for sentinel node detection: (99m)Tc-DTPA-mannosyl-dextran. J Nucl Med.
6 Torabi M., Aquino S.L., Harisinghani M.G. (2004). Current concepts in lymph node imaging. J Nucl Med.
7 Schoder H., Glass E.C., Pecking A.P., Harness J.K., Wallace A.M., Hirnle P., Alberini J.L., Vilain D., Larson S.M., Hoh C.K., Vera D.R. (2006). Molecular targeting of the lymphovascular system for imaging and therapy. Cancer Metastasis Rev.
8 Luciani A., Itti E., Rahmouni A., Meignan M., Clement O. (2006). Lymph node imaging: basic principles. Eur J Radiol.
9 Wunderbaldinger P. (2006). Problems and prospects of modern lymph node imaging. Eur J Radiol.
10 Qian C.N., Berghuis B., Tsarfaty G., Bruch M., Kort E.J., Ditlev J., Tsarfaty I., Hudson E., Jackson D.G., Petillo D., Chen J., Resau J.H., Teh B.T. (2006). Preparing the "soil": the primary tumor induces vasculature reorganization in the sentinel lymph node before the arrival of metastatic cancer cells. Cancer Res.
11 Harrell M.I., Iritani B.M., Ruddell A. (2007). Tumor-induced sentinel lymph node lymphangiogenesis and increased lymph flow precede melanoma metastasis. Am J Pathol.
12 Dadras S.S., Lange-Asschenfeldt B., Velasco P., Nguyen L., Vora A., Muzikansky A., Jahnke K., Hauschild A., Hirakawa S., Mihm M.C., Detmar M. (2005). Tumor lymphangiogenesis predicts melanoma metastasis to sentinel lymph nodes. Mod Pathol.
13 Van den Eynden G.G., Vandenberghe M.K., van Dam P.J., Colpaert C.G., van Dam P., Dirix L.Y., Vermeulen P.B., Van Marck E.A. (2007). Increased sentinel lymph node lymphangiogenesis is associated with nonsentinel axillary lymph node involvement in breast cancer patients with a positive sentinel node. Clin Cancer Res.
14 Jiang D., Liang J., Noble P.W. (2011). Hyaluronan as an immune regulator in human diseases. Physiol Rev.
15 Sironen R.K., Tammi M., Tammi R., Auvinen P.K., Anttila M., Kosma V.M. (2011). Hyaluronan in human malignancies. Exp Cell Res.
16 Aruffo A., Stamenkovic I., Melnick M., Underhill C.B., Seed B. (1990). CD44 is the principal cell surface receptor for hyaluronate. Cell.
17 Mumprecht V., Honer M., Vigl B., Proulx S.T., Trachsel E., Kaspar M., Banziger-Tobler N.E., Schibli R., Neri D., Detmar M. (2010). In vivo imaging of inflammation- and tumor-induced lymph node lymphangiogenesis by immuno-positron emission tomography. Cancer Res.